# ^64^Cu-4,11-bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-LLP2A

Chemical name: | ^64^Cu-4,11-bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-LLP2A
Abbreviated name: | ^64^Cu-CB-TE2A-LLP2A
Synonym:
Agent category: | Peptide
Target: | Integrin α_4_β_1_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=119631392), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=67191026) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3676) for more information about integrin α_4_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A)]

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_4_β_1_ integrin plays an important role in hematopoiesis of lymphocytes. On the other hand, it affects tumor growth, tumor invasiveness and metastasis (2). The α_4_β_1_ integrin is strongly expressed on lymphoid tumor cells (3). N-[[4-[[[(2-ethylphenyl)amino]carbonyl]amino]phenyl]acetyl]-N(epsilon)-6-[(2E)-1-oxo-3-(3-pyridinyl-2-propenyl)]-L-lysyl-L-2-aminohexanedioyl-(1-amino-1-cyclohexane)carboxamide (LLP2A) was identified as a tripeptide peptidomimetic ligand to bind to α_4_β_1_ integrin on human Jurkat T-lymphoid leukemia cells using “one-bead one compound” combinatorial libraries (4). LLP2A was conjugated with Alexa Fluor 680 (Alexa680) via biotin and streptavidin (SA) interaction to study in vivo biodistribution of the tracer in tumor-bearing mice (4). LLP2A-SA-Alexa680 was found to have a high specific accumulation in α_4_β_1_-positve lymphoid tumor cells in nude mice. DeNardo et al. (5) has prepared ^64^Cu-bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-LLP2A (^64^Cu-CB-TE2A-LLP2A) for use in positron emission tomography (PET) imaging of α_4_β_1_ expression in tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+synthesis)]

CB-TE2A-LLP2A (1.8 kDa) was obtained using solid-phase synthesis (5). Fmoc-Lys(Dde)-OH was first coupled to the resin, then 2 linkers were coupled to Lys(Dde). LLP2A was assembled on the N terminus of the linker. CB-TE2A was coupled to the side chain of Lys(Dde). Radiolabeling was performed by mixing ^64^CuCl_2_ with CB-TE2A-LLP2A. The mixture in 0.14 M ammonium acetate (pH 7) was heated at 95ºC for 60 min. The radiochemical purity and specific activity of ^64^Cu-CB-TE2A-LLP2A were >99% and 666 MBq/µmol (18 mCi/µmol), respectively. The labeling yield was 75-90%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+and+in+vitro)]

An in vitro receptor-binding assay of ^111^In-DOTA-LLP2A was performed on α_4_β_1_ integrin expressing human Raji lymphoma cell line (5). There were 1.7x10^5^ sites/cell with an association constant value of 2 x 10^8^ M^-1^. Binding of ^64^Cu-CB-TE2A-LLP2A (1 ng/10^6^ cells) to α_4_β_1_ integrin was 35% of the incubation dose after 60 min of incubation at room temperature. Peng et al. (4) showed that LLP2A binds to α_4_β_1_, but not to α_v_β_1_, α_v_β_3_, α_3_β_1_ α_2_β_1_, α_6_β_1_, α_9_β_1_ (closely related to α_4_β_1_), α_L_β_2_ and α_M_β_2_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+rodentia)]

DeNardo et al. (5) performed PET imaging studies of ^64^Cu-CB-TE2A-LLP2A in nude mice bearing a Raji subcutaneous xenograft. Images were obtained after injection of 1.1 nmol/mouse of ^64^Cu-CB-TE2A-LLP2A at 4 and 24 h after injection. Only the tumor and spleen were clearly visualized as observed in these two time points of measurement. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+human)]

No publication is currently available.

## NIH Support

U19 113298, U24 CA110804

## References

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Holzmann B., Gosslar U., Bittner M. (1998). alpha 4 integrins and tumor metastasis. Curr Top Microbiol Immunol.
3 Vincent A.M., Cawley J.C., Burthem J. (1996). Integrin function in chronic lymphocytic leukemia. Blood.
4 Peng L., Liu R., Marik J., Wang X., Takada Y., Lam K.S. (2006). Combinatorial chemistry identifies high-affinity peptidomimetics against alpha4beta1 integrin for in vivo tumor imaging. Nat Chem Biol.
5 Denardo S.J., Liu R., Albrecht H., Natarajan A., Sutcliffe J.L., Anderson C., Peng L., Ferdani R., Cherry S.R., Lam K.S. (2009). 111In-LLP2A-DOTA Polyethylene Glycol-Targeting {alpha}4{beta}1 Integrin: Comparative Pharmacokinetics for Imaging and Therapy of Lymphoid Malignancies. J Nucl Med.